# ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-c(D-Cys-Phe-Tyr-D-AgI^8^(Me,2-naphthoyl)-Lys-Thr-Phe-Cys)-OH

Chemical name: | ^111^In-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-c(D-Cys-Phe-Tyr-D-Agl^8^(Me,2-naphthoyl)-Lys-Thr-Phe-Cys)-OH
Abbreviated name: | ^111^In-DOTA-sst_3_-ODN-8
Synonym:
Agent category: | Peptide
Target: | Somatostatin receptor (sst_3_)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=47117741), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=71979669) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6750) for more information about somatostatin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8)]

Somatostatin (SST) is an inhibitor of the release of somatotropin, glucagon, insulin, gastrointestinal hormones, and other secretory proteins (1). SST is also known as somatotropin release-inhibiting factor (SRIF). SST is a cyclic polypeptide with two biologically active isoforms, SRIF-14 and SRIF-28, of 14 and 28 amino acids, respectively. SRIF has a short plasma half-life of <3 min (2). SST receptors (SSTRs) (G-protein–coupled) have been found on a variety of neuroendocrine tumors and cells of the immune system, and five individual subtypes (sst_1_–sst_5_) have been identified and subsequently cloned from animal and human tissues (3, 4). SST also inhibits cell proliferation and promotes apoptosis through binding to specific cell-surface SSTRs (5).

^111^In-Labeled diethylenetriaminepentaacetic acid-octreotide (^111^In-DTPA-OCT) is an SST analog that, over the last decade, has remained the most widely used radiopharmaceutical for the scintigraphic detection and staging of primary and metastatic neuroendocrine tumors bearing SSTRs with single-photon emission computed tomography (SPECT) (6). It has also shown promising results in peptide-receptor radionuclide therapy (7). Octreotide (OCT) is a cyclic peptide with eight amino acids. ^111^In-DTPA-OCT binds with high affinity to SSTR subtypes 2 and 5 (sst_2_ and sst_5_) and to sst_3_ to a lesser degree, but it does not bind to sst_1_ and sst_4_ (8). Currently used targeting SSTR peptides mainly have affinity for sst_2_. However, sst_1_, sst_3_, sst_4_, and sst_5_ are also expressed in different tumors. Therefore, there is a need for pansomatostatin radioligands (9). Ginj et al. (10) have developed a series of sst_3_ antagonist ligands. One of them, c(D-Cys-Phe-Tyr-D-Agl^8^(Me,2-naphthoyl)-Lys-Thr-Phe-Cys)-OH (sst_3_-ODN-8), was found to be a selective sst_3_ antagonist. For evaluation as a SPECT imaging agent for sst_3_, ^111^In has been attached to sst_3_-ODN-8 via tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^111^In-DOTA-sst_3_-ODN-8.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8+and+synthesis)]

DOTA-sst_3_-ODN-8 was synthesized via standard solid-phase peptide synthesis (10). DOTA was incorporated at the N-terminus of the peptide. DOTA-sst_3_-ODN-8 was purified with high-performance liquid chromatography. Neither the radiolabeling procedure for DOTA-sst_3_-ODN-8 with ^111^In nor the radiochemical yield or radiochemical purity was reported. ^111^In-DOTA-sst_3_-ODN-8 had a specific activity of ~20 GBq/µmol (0.54 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8+and+in+vitro)]

^111^In-DOTA-sst_3_-ODN-8 showed a B_max_ (receptor density) of 5,180 pmol/mg protein in HEK-sst_3_ cells (10). On the other hand, ^111^In-DOTA-NOC (sst_2_, sst_3_, and sst_5_ agonist) exhibited a B_max_ of 68 pmol/mg protein. Hence, the antagonist labeled 75-fold more sst_3_ receptor sites than the agonist. DOTA-sst_3_-ODN-8 showed 50% inhibition concentration (IC_50_) values of >1,000, 5.2 ± 1.3, >1,000, >1,000, and >1,000 nM for human sst_1_, sst_2_, sst_3_, sst_4_, and sst_5_ receptors in competition with ^125^I-SRIF-28, respectively. DOTA-sst_3_-ODN-8 was not internalized in cultured HEK-sst_3_ cells, whereas In-DOTA-NOC and SRIF-28 were internalized. However, DOTA-sst_3_-ODN-8 inhibited the internalization of the two agonists.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8+and+rodentia)]

Ginj et al. (10) performed ex vivo biodistribution studies with 0.2 MBq (5.4 µCi, 0.01 nmol) ^111^In-DOTA-sst_3_-ODN-8 in HEK-sst_3_ tumor-bearing nude mice (n = 3/group). The accumulation of radioactivity in the sst_3_ tumors was 22.1% injected dose per gram (% ID/g) at 0.25 h, 34.8% ID/g at 0.5 h, 61.3% ID/g at 1 h, 49.7% ID/g at 4 h, and 30.8% ID/g at 24 h after injection. The kidney was the organ that had the highest accumulation (15.8% ID/g) at 1 h after injection, followed by the pituitary (5.3% ID/g), blood (1.8% ID/g), liver (1.3% ID/g), and pancreas (0.5% ID/g). Accumulation of radioactivity in the other tissues was low. The concentration in the blood was 0.1% ID/g at 4 h after injection, with tumor/blood ratios of 34, 497, and 1,026 at 1, 4, and 24 h, respectively. Tumor/muscle ratios were 68, 248, and 342 at 1, 4, and 24 h, respectively. Co-injection with sst_3_-ODN-8 (50 nmol) reduced the accumulation of radioactivity by 60% in the tumors, 20% in the adrenal, 28% in the pancreas, and 70% in the pituitary at 15 min after injection. Little or no inhibition was observed in the stomach, kidney, spleen, liver, and bone. On the other hand, accumulation of ^111^In-DOTA-NOC was only 17.5, 6.5, and 3.5% ID/g at 0.5, 1, and 24 h, respectively. The accumulation of the agonist was less than the antagonist in the sst_3_ tumors. Co-injection with In-DOTA-NOC (50 nmol) reduced the accumulation of radioactivity by 37% in the tumors, 86% in the stomach, 80% in the adrenal, 90% in the pancreas, and 60% in the pituitary at 4 h after injection. Mice bearing both the HEK-sst_2_ and the HEK-sst_3_ tumors were injected with ^111^In-DOTA-sst_3_-ODN-8 or ^111^In-DOTA-NOC, whole-body SPECT imaging was performed. The HEK-sst_3_ tumor was clearly visualized with ^111^In-DOTA-sst_3_-ODN-8 at 0.5 and 4 h after injection, but the HEK-sst_2_ tumor was not. On the other hand, ^111^In-DOTA-NOC showed only a weak accumulation in both tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=sst(3)-ODN-8+and+human)]

No publication is currently available.

## NIH Support

R01 DK59953

## References

1 Weckbecker G., Lewis I., Albert R., Schmid H.A., Hoyer D., Bruns C. (2003). Opportunities in somatostatin research: biological, chemical and therapeutic aspects. Nat Rev Drug Discov.
2 Patel Y.C., Wheatley T. (1983). In vivo and in vitro plasma disappearance and metabolism of somatostatin-28 and somatostatin-14 in the rat. Endocrinology.
3 Corleto V.D., Nasoni S., Panzuto F., Cassetta S., Delle Fave G. (2004). Somatostatin receptor subtypes: basic pharmacology and tissue distribution. Dig Liver Dis.
4 Moller L.N., Stidsen C.E., Hartmann B., Holst J.J. (2003). Somatostatin receptors. Biochim Biophys Acta.
5 Barnett P. (2003). Somatostatin and somatostatin receptor physiology. Endocrine.
6 Krenning E.P., Kwekkeboom D.J., Bakker W.H., Breeman W.A., Kooij P.P., Oei H.Y., van Hagen M., Postema P.T., de Jong M., Reubi J.C., et al. (1993). Somatostatin receptor scintigraphy with [111In-DTPA-D-Phe1]- and [123I-Tyr3]-octreotide: the Rotterdam experience with more than 1000 patients. Eur J Nucl Med.
7 Kwekkeboom D.J., Mueller-Brand J., Paganelli G., Anthony L.B., Pauwels S., Kvols L.K. (2005). M. O'Dorisio T, R. Valkema, L. Bodei, M. Chinol, H.R. Maecke, and E.P. Krenning, Overview of results of peptide receptor radionuclide therapy with 3 radiolabeled somatostatin analogs. J Nucl Med.
8 Storch D., Behe M., Walter M.A., Chen J., Powell P., Mikolajczak R., Macke H.R. (2005). Evaluation of [99mTc/EDDA/HYNIC0]octreotide derivatives compared with [111In-DOTA0,Tyr3, Thr8]octreotide and [111In-DTPA0]octreotide: does tumor or pancreas uptake correlate with the rate of internalization?. J Nucl Med.
9 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
10 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.